# ^99m^Tc-Hydrazinonicotinamide-chitosan-anti-vascular endothelial growth factor receptor 2 monoclonal antibody DC101

Chemical name: | ^99m^Tc-Hydrazinonicotinamide-chitosan- anti-vascular endothelial growth factor receptor 2 monoclonal antibody DC101
Abbreviated name: | ^99m^Tc-HYNIC-chitosan-DC101
Synonym:
Agent category: | Antibody
Target: | Vascular endothelial growth factor receptor 2 (VEGFR-2)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal/contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=9087218), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/229892299) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=3791) for more information about VEGFR-2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DC101%20chitosan)]

Vascular endothelial growth factor (VEGF) consists of at least six isoforms with various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (1). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species (2). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFRs) on endothelial cells (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4). Several types of non-endothelial cells such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells also express VEGFRs (1).

VEGFRs have been found to be overexpressed in various tumor cells and tumor-associated endothelial cells (3). Inhibition of VEGFR function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (4, 5). Radiolabeled VEGF has been developed as a tracer for imaging solid tumors and angiogenesis in humans (6-8). Chitosan is a linear polysaccharide composed of D-glucosamine and N-acetylglucosamine subunits with numerous amine groups in D-glucosamine for ligand conjugation. A rat anti-VEGFR-2 monoclonal antibody (mAb), DC101, has been shown to inhibit angiogenesis with suppression of tumor growth and metastasis. Lee et al. (9) conjugated DC101 mAb to hydrazinonicotinamide (HYNIC)-chitosan for radiolabeling with ^99m^Tc to form ^99m^Tc-HYNIC-chitosan-DC101 for imaging VEGFR-2 expression under ischemic conditions.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DC101%20chitosan+synthesis)]

Deacetylated chitosan (5 kDa) was incubated with succinimidyl HYNIC in 0.2 M borate buffer (pH 8.2) for 6 h at room temperature (9). HYNIC-chitosan was isolated with ultracentrifugation. DC101 mAb or human IgG (6.6 nM) was incubated with 20 mM sodium meta-periodate for 30 min at 4°C. The periodate-oxidized mAb and HYNIC-chitosan were incubated in the presence of sodium cynoborohydride for 2 h at 4°C. HYNIC-chitosan-DC101 conjugates were isolated with ultracentrifugation. The molecular weights of DC101 and HYNIC-chitosan-DC101 were found with MALDI-TOF mass spectroscopy to be 144.7 and 150.6 kDa, respectively. The number of amine groups that were conjugated was not reported.

HYNIC-chitosan-DC101 conjugates (1.3 nmol) were incubated with 46.3 MBq (1.25 mCi) ^99m^Tc-sodium pertechnetate, tricine, and stannous chloride for 30 min at room temperature. ^99m^Tc-HYNIC-chitosan-DC101 conjugates were isolated with column chromatography with >95% labeling efficiency and was stable in serum for 6 h. The specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DC101%20chitosan+in+vitro)]

In vitro binding tests showed binding of FITC-chitosan-DC101 (0.13 nmol) to human umbilical vein endothelial cells (HUVECs) expressing VEGFR-2. Confocal microscopy showed that most of the FITC-chitosan-DC101 bound to the cytosol of HUVECs after 2 h of incubation (9). In contrast, FITC-chitosan-IgG control did not bind to the cells. Flow cytometry analysis showed that FITC-chitosan-DC101 binding to the cells exhibited ~10-fold greater fluorescent intensity than FITC-chitosan-IgG binding.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DC101%20chitosan+rodentia)]

Lee et al. (9) performed single-photon emission computed tomography scintigraphic imaging using an ischemic mouse model. Images were captured after intravenous injection of 18.5 MBq (0.5 mCi) ^99m^Tc-HYNIC-chitosan-DC101 at 2, 12, and 24 h after artery ligation. The accumulation of radioactivity was similar in the ischemic hindlimb and contralateral hindlimb at 2 h after operation but continued to increase in the ischemic hindlimb at 12 h and 24 h after operation. On the other hand, the ^99m^Tc-HYNIC-chitosan-IgG control did not show any significant accumulation in the ischemic hindlimb. The ischemic tissue/normal tissue ratios at 24 h after injection were 4.5 ± 0.25 for the DC101 conjugates and 1.6 ± 0.56 for the IgG control conjugates. Ex vivo biodistribution studies were performed at 3 h after injection of ^99m^Tc-HYNIC-chitosan-DC101 in ischemic mice (n = 4/group) at 12 h and 24 h after operation.Tracer accumulation in the ischemic muscle was 2.39 ± 0.87% injected dose per gram (ID/g) at 12 h and 3.03 ± 0.80% ID/g at 24 h. The ischemic tissue/normal tissue ratios were 2.65 and 1.91 at 12 h and 24 h, respectively. There was an increase of VEGFR-2 expression with time in the ischemic tissues. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DC101%20chitosan+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DC101%20chitosan+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DC101%20chitosan+human)]

No publication is currently available.

## References

1 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
2 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
3 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
4 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
5 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
6 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
7 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
9 Lee, C.M., E.M. Kim, S.J. Cheong, D.W. Kim, S.T. Lim, M.H. Sohn, and H.J. Jeong, Targeted molecular imaging of VEGF receptors overexpressed in ischemic microvasculature using chitosan-DC101 conjugates. J Biomed Mater Res A, 2009